# (S,S)-2-[α-(2-(2-[^18^F]Fluoroethoxy)phenoxy)benzyl]morpholine

Chemical name: | (S,S)-2-[α-(2-(2-[^18^F]Fluoroethoxy)phenoxy)benzyl]morpholine
Abbreviated name: | (S,S)-[^18^F]FRB
Synonym: | (S,S)-[^18^F]Fluororeboxetine, [^18^F]FRB
Agent Category: | Compound
Target: | Brain norepinephrine transporter (NET)
Target Category: | Transporter binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFRB%20OR%20%28%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29)]

(S,S)-2-[α-(2-(2-[^18^F]Fluoroethoxy)phenoxy)benzyl]morphine ((S,S)-[^18^F]FRB) is a radioligand developed for positron emission tomography (PET) imaging of the brain adrenergic receptors (1, 2). It is a derivative of reboxetine ((RS)-2-[(RS)-2-ethoxyphenoxy)benzyl]morpholine), a norepinephrine (NE) transporter (NET) inhibitor, labeled with ^18^F, a positron emitter with a physical half-life (t_½_) of 109.8 min.

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (3, 4). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter NE, which stimulates adrenergic receptors in various effector organs (5). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (6). All NE receptors belong to the G-protein−linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NET is a transmembrane protein located in the adrenergic nerve terminals and is responsible for active reuptake (uptake-1) of NE released from neurons (7). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. Brain NETs are involved in various neurologic and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (8). Brain NETs are also the site of action of many antidepressant drugs in the brain (9).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in patients with various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (6). [^123^I]-meta-Iodobenzylguanidine, [^11^C]meta-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (10). However, this class of tracers is not suitable for the study of brain NET system because they are not able to cross the blood-brain barrier (2). In the brain, NET levels are relatively lower than other receptors, such as dopamine transporters (DATs) and serotonin transporters (9). Several NET reuptake inhibitors, such as [^11^C]desipramine, have been tested, but they showed high nonspecific binding. Reboxetine is a specific NET inhibitor with a high affinity and selectivity [inhibitory concentration (IC_50_) DAT/NET = 4,000]. ^11^C-labeled reboxetine derivatives ((S,S)-[^11^C]methylreboxetine((S,S)-[^11^C]MRB)) have shown specific localization and favorable binding kinetics in rats and non-human primates with PET imaging (11). Because of the potential advantages associated with the longer t_½_ of ^18^F, Lin et al. (1) synthesized a number of ^18^F labeled reboxetine analogs as promising radioligands for NET imaging with PET.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20synthesis)]

Lin et al. (11) described the radiosynthesis of (S,S)-[^18^F]FRB from (S,S)-N-tert-butyloxycarbonyl-2-[α-(2-hydroxyphenoxy)benzyl]morpholine (N-Boc-desethylIRB). N-Boc-desethylIRB was prepared by the N-protection of (S,S)/(R,R)-N-desethylIRB with a tert-butyloxycarbonyl (Boc) group followed by enantiomeric resolution by chiral HPLC with >99% enantiomeric purity. In the radiosynthesis, 1-bromo-2-[^18^F]fluoroethane ([^18^F]BFE) was first prepared as a secondary radiolabeling synthon by the nucleophilic displacement of 2-bromoethyl triflate with [^18^F]F−. Briefly, 2-bromoethyl triflate was added to [^18^F]KF/Kryptofix 222 and vortexed for 20 s, followed by incubation at ambient temperature for 5 min. The solution was heated at 80ºC, and the volatiles were distilled into a solution of N-Boc-desethylIRB and 5 N sodium hydroxide in N,N-dimethylformamide cooled in an acetonitrile/dry ice bath. This step produced the coupling of N-Boc-desethylIRB with [^18^F]BFE.The mixture was then heated in an oil bath at 130ºC for 30 min. After cooling, trifluoroacetic acid was added to remove the Boc group and heated at 75ºC for 17 min. Water was added and (S,S)-[^18^F]FRB was purified by high performance liquid chromatography (HPLC). After HPLC purification, (S,S)-[^18^F]FRB was obtained in 11−27% decay-corrected radiochemical yields from [^18^F]F−. The total synthesis time was 120 min with a radiochemical purity of >98%. The specific activity of the final product was 21−48 GBq (0.57−1.3 Ci)/μmol at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20in%20vitro)]

Lin et al. (1) determined the log P_oct_ (pH 7.4) value of FRB to be 0.91 ± 0.01 (n = 8) by traditional extraction with octanol and pH 7.4 phosphate buffer. In comparison, (S,S)-[^11^C]MRB had log P of 1.17.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20rodentia)]

Whole-body biodistribution studies of (S,S)-[^18^F]FRB were conducted in mice (1). At 10 min after i.v. injection of 0.185 MBq (5 μCi) (S,S)-[^18^F]FRB, the percent injected dose per gram (%ID/g; n = 4) radioactivity levels for major organs were 17.5 ± 1.43 (liver), 9.99 ± 0.55 (intestine), 5.54 ± 1.07 (kidney), 4.52 ± 1.14 (lung), 1.74 ± 0.08 (bone), 1.31 ± 0.07 (blood), and 0.42 ± 0.03 (brain), At 2 h, these radioactivity levels changed to 5.82 ± 1.16 (liver), 30.7 ± 1.78 (intestine), 0.77 ± 0.11 (kidney), 0.31 ± 0.03 (lung), 0.83 ± 0.04 (bone), 0.44 ± 0.03 (blood), and 0.16 ± 0.01 (brain), The results showed that the radioligand was excreted through both hepatobiliary and renal systems. There was a moderate brain radioactivity uptake and the washout was slow. In comparison, (S,S)-[^11^C]MRB had 0.53% ID brain uptake at 5 min after injection (9). The bone radioactivity level decreased initially but there appeared to be a slight increase from 1 h (0.65% ID) to 2 h (0.83% ID). This might indicate evidence of in vivo defluorination.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20%28primate%20NOT%20human%29)]

Ding et al. (12) used PET imaging to evaluate (S,S)-[^18^F]FRB in baboons. The radioactivity uptake of (S,S)-[^18^F]FRB in the baboon brain was consistent with the known NET distribution, and the uptake could be blocked by a selective NET inhibitor (i.y. nisoxetine pretreatment, 1 mg/kg). In comparison, no regional specificity or blocking effect was observed for the (R,R)-[ ^18^F]FRB. The peak brain uptake and signal to noise ratio [distribution volume ratio DVR _(TH/Ref)_] of (S,S)-[^18^F]FRB were 1.8% ID and 1.3-1.6, respectively. The results of the HPLC analysis and solid-phase extraction of the baboon plasma samples showed that (R,R)-[ ^18^F]FRB was metabolized faster than (S,S)-[^18^F]FRB. The plasma protein binding (% unbound) of (S,S)-[^18^F]FRB was 13. The %unchanged parent compound was 96% at 1 min and 20% at 120 min. (S,S)-[^18^F]FRB displayed relatively fast kinetics in NET-rich brain regions, which might facilitate its central nervous system kinetic analysis.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFRB%20OR%20%5B18F%5Dfluororeboxetine%20OR%20%28fluorinated%20reboxetine%20analog%29%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH NIBIB EB002630, NIH NIDA DA-06278.

## References

1 Lin K.S., Ding Y.S., Kim S.W., Kil K.E. (2005). Synthesis, enantiomeric resolution, F-18 labeling and biodistribution of reboxetine analogs: promising radioligands for imaging the norepinephrine transporter with positron emission tomography. Nucl Med Biol.
2 Ding Y.S., Lin K.S., Logan J., Benveniste H., Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
3. Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
4. Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
5. Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
6. Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
7 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
8 Zahniser N.R., Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
9 Wilson A.A., Johnson D.P., Mozley D., Hussey D., Ginovart N., Nobrega J., Garcia A., Meyer J., Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
10 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
11 Lin K.S., Ding Y.S. (2004). Synthesis, enantiomeric resolution, and selective C-11 methylation of a highly selective radioligand for imaging the norepinephrine transporter with positron emission tomography. Chirality.
12 Link J.M., Synovec R.E. (1999). Whole-column radioactivity detection: simultaneous separation and enhanced detectability. Anal Chem.